# 18-[^18^F]Fluoro-4-thia-palmitate

Chemical name: | 18-[^18^F]Fluoro-4-thia-palmitate
Abbreviated name: | [^18^F]FTP
Synonym:
Agent category: | Compound
Target: | Fatty acid oxidation (FAO) enzymes
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP)]

β-Oxidation of long-chain fatty acids is the major (60%–80%) aerobic process for energy production in the heart, liver, and skeletal muscle. Abnormalities of fatty acid oxidation (FAO) are associated with several cardiovascular diseases, neurodegeneration, fatty liver, and diabetes (1-5). Myocardium has a high mitochondrial content because of high energy usage. Carnitine palmitoyltransferases (CPT1 and CPT2) mediate transfer of fatty acids into the mitochondrial matrix for β-oxidation (6, 7). Various radiolabeled, thia-substituted, fatty acid analogs have been found to be metabolically trapped in the myocardial mitochondria (8-10). 4-Thia fatty acids are oxidized in the mitochondria to 4-thia-enoyl-CoAs, which cannot be further metabolized and trapped (protein-bound) in the mitochondria. DeGrado et al. (11, 12) have synthesized 18-[^18^F]fluoro-4-thia-palmitate ([^18^F]FTP) for evaluation as a positron emission tomography (PET) agent of FAO.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Fatty%20acid%20oxidation%20AND+micad%5Bbook%5D)
- Gene information in NCBI (CPT1 (http://www.ncbi.nlm.nih.gov/gene/1374))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/600528)
- Clinical trials (CPT1 (http://www.clinicaltrials.gov/ct2/results?term=Carnitine+palmitoyltransferase))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP+synthesis)]

[^18^F]FTP was prepared as described by DeGrado et al. (13). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and methyl-16-iodo-4-thia-hexadecanoate were heated in acetonitrile for 15 min at 85°C, followed by hydrolysis with KOH for 4 min at 90°C. [^18^F]FTP was purified with high-performance liquid chromatography with radiochemical yields of 25%–60% (decay-corrected) and a radiochemical purity of >99%. Specific activity of [^18^F]FTP was >74.0 GBq/µmol (2.0 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP%20and%20in%20vitro)]

DeGrado et al. (13) performed perfusion studies with isolated rat hearts (n = 5 per group) in normoxic (95% O_2_) and hypoxic (35% O_2_) conditions. [^18^F]FTP was administered at the aortic root. The fractional tracer metabolic rate (FR_FTP_) was 1.45 ± 0.39 mL/min per g under normoxic conditions and 0.73 ± 0.16 mL/min per g under hypoxic conditions. There was a reduction of 50% in the hypoxic group relative to the normoxic group. The FR_FTP_ was ~60% of the palmitate oxidation rate in these two conditions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP%20and%20rodentia)]

DeGrado et al. (12) performed ex vivo biodistribution studies of [^18^F]FTP in rats. [^18^F]FTP accumulated mainly in the heart, liver, bone, and kidney with 0.32 ± 0.17% injected dose (ID)/g, 1.15 ± 0.16% ID/g, 0.24 ± 0.07% ID/g, and 0.25 ± 0.04% ID/g, respectively, at 30 min after injection. Retention of [^18^F]FTP in the heart was moderate with 0.17 ± 0.05% ID/g at 120 min, whereas there was a slight washout in the liver and kidney. Bone accumulation was approximately one-fold higher at 120 min. Pretreatment with the CPT1 inhibitor etomoxir (40 mg/kg, 120 min before [^18^F]FTP injection) reduced the radioactivity level in the heart by 82% at 30 min after injection with little inhibition in the other organs. Folch-type analysis of the excised hearts showed that 80% of [^18^F]FTP radioactivity was protein-bound. Pretreatment with etomoxir reduced the protein-bound radioactivity to 10%. The heart/blood, heart/lung, heart/brain, and heart/muscle ratios were 7, 3, 10, and 10, respectively, at 120 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20FTP+and+(dog+or+pig+or+sheep+or+rabbit))]

Whole-body PET imaging in two swine showed that [^18^F]FTP accumulated mainly in the heart, liver, and kidneys with low accumulation in the bone over an imaging period of 3 h (13). Good myocardial images were observed at 10–20 min after injection with little interference from the lung and liver. Myocardium/blood and myocardium/lung ratios were 7 and 8, respectively, at 20 min after injection. Myocardium clearance half-time of radioactivity was 5 h, whereas the clearance half-time was 50 min for the liver.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FTP%20and%20human)]

No publication is currently available.

## NIH Support

R01 HL63371, R01 CA108620, HL54882

## References

1 Stanley W.C., Recchia F.A., Lopaschuk G.D. (2005). Myocardial substrate metabolism in the normal and failing heart. Physiol Rev.
2 Bergmann S.R., Herrero P., Sciacca R., Hartman J.J., Rubin P.J., Hickey K.T., Epstein S., Kelly D.P. (2001). Characterization of altered myocardial fatty acid metabolism in patients with inherited cardiomyopathy. J Inherit Metab Dis.
3 Liu Y. (2006). Fatty acid oxidation is a dominant bioenergetic pathway in prostate cancer. Prostate Cancer Prostatic Dis.
4 You M., Crabb D.W. (2004). Recent advances in alcoholic liver disease II. Minireview: molecular mechanisms of alcoholic fatty liver. Am J Physiol Gastrointest Liver Physiol.
5 Stanley W.C., Lopaschuk G.D., McCormack J.G. (1997). Regulation of energy substrate metabolism in the diabetic heart. Cardiovasc Res.
6 Jogl G., Hsiao Y.S., Tong L. (2004). Structure and function of carnitine acyltransferases. Ann N Y Acad Sci.
7 Bonnefont J.P., Djouadi F., Prip-Buus C., Gobin S., Munnich A., Bastin J. (2004). Carnitine palmitoyltransferases 1 and 2: biochemical, molecular and medical aspects. Mol Aspects Med.
8 Taylor M., Wallhaus T.R., Degrado T.R., Russell D.C., Stanko P., Nickles R.J., Stone C.K. (2001). An evaluation of myocardial fatty acid and glucose uptake using PET with [18F]fluoro-6-thia-heptadecanoic acid and [18F]FDG in Patients with Congestive Heart Failure. J Nucl Med.
9 DeGrado T.R., Wang S., Rockey D.C. (2000). Preliminary evaluation of 15-[18F]fluoro-3-oxa-pentadecanoate as a PET tracer of hepatic fatty acid oxidation. J Nucl Med.
10 Stone C.K., Pooley R.A., DeGrado T.R., Renstrom B., Nickles R.J., Nellis S.H., Liedtke A.J., Holden J.E. (1998). Myocardial uptake of the fatty acid analog 14-fluorine-18-fluoro-6-thia-heptadecanoic acid in comparison to beta-oxidation rates by tritiated palmitate. J Nucl Med.
11 DeGrado T.R., Bhattacharyya F., Pandey M.K., Belanger A.P., Wang S. (2010). Synthesis and preliminary evaluation of 18-(18)F-fluoro-4-thia-oleate as a PET probe of fatty acid oxidation. J Nucl Med.
12 DeGrado T.R., Kitapci M.T., Wang S., Ying J., Lopaschuk G.D. (2006). Validation of 18F-fluoro-4-thia-palmitate as a PET probe for myocardial fatty acid oxidation: effects of hypoxia and composition of exogenous fatty acids. J Nucl Med.
13 DeGrado T.R., Wang S., Holden J.E., Nickles R.J., Taylor M., Stone C.K. (2000). Synthesis and preliminary evaluation of (18)F-labeled 4-thia palmitate as a PET tracer of myocardial fatty acid oxidation. Nucl Med Biol.